# ^89^Zr-Labeled trastuzumab, a humanized monoclonal antibody against epidermal growth factor receptor 2

Chemical name: | ^89^Zr-Labeled trastuzumab, a humanized monoclonal antibody against epidermal growth factor receptor 2
Abbreviated name: | ^89^Zr-Trastuzumab
Synonym:
Agent Category: | Antibody
Target: | Epidermal growth factor receptor 2 (EGFR2)
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^89^Zr
Activation: | No
Studies: | - In vitro; - Rodents | Structural information is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=trastuzumab&cmd=DetailsSearch)]

Trastuzumab (http://www.cancer.gov/cancertopics/druginfo/trastuzumab), a humanized monoclonal antibody (mAb) that targets epidermal growth factor receptor 2 (HER2), is commercially available in the United States (US) and is approved (http://www.cancer.gov/cancertopics/druginfo/fda-trastuzumab) by the US Food and Drug Administration for the treatment of HER2-overexpressing breast cancer (BC). This immunopharmaceutical is also being evaluated in combination with other anti-cancer drugs in clinical trials (http://clinicaltrials.gov/ct2/results?term=trastuzamab) for the treatment of metastatic BC. In the clinical setting, the overexpression or amplification of HER2 is determined in tumor biopsies and indicates a poor prognostic outcome for the BC patient (1). Usually, the HER2 status of a tumor is established in the primary tumor after a biopsy, but the HER2 levels may not be the same at all locations in the tumor, and the receptor levels can change after the initiation of BC therapy (2). Although repeated determination of HER2 levels in tumor biopsies during the course of therapy could be a good indicator of treatment effectiveness, taking biopsies is an invasive process, and clinicians and patients are averse to using this technique. In addition, it is difficult to biopsy small and inaccessible tumors of the patient (1).

Recently, as an alternative to biopsies, whole-body HER2 immunoscintigraphy with ^111^In-labeled trastuzumab using single-photon emission computed tomography (SPECT) was shown to be a suitable non-invasive technique for the detection of HER2-positive xenograft tumors in mice (3). Using SPECT, tumors could also be detected in patients with BC (4). In an effort to develop a HER2 imaging agent with superior spatial resolution and signal/noise ratio compared to ^111^In-trastuzumab, Dijkers et al. (1) developed ^89^Zr-labeled trastuzumab (^89^Zr-trastuzumab; ^89^Zr has a half-life of 78.41 hr)) for use with positron emission tomography (PET). The ^89^Zr-labeled mAb was then evaluated for the detection of HER2-positive xenograft tumors in mice, and results obtained with this labeled mAb were compared with those obtained with ^111^In-trastuzumab using SPECT (1).

### Other sources of information regarding EGFR

Other EGFR imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad).

Human EGFR ligands (http://www.ncbi.nlm.nih.gov/pubmed?term=Human%20EGFR%20ligands&cmd=DetailsSearch) in PubMed.

Human EGFR on OMIM (http://www.ncbi.nlm.nih.gov/omim?term=Human%20EGFR) (Online Mendelian Inheritance in Man).

Human EGFR gene (http://www.ncbi.nlm.nih.gov/protein?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=1956&log$=genesensor5&logdbfrom=protein).

Protein (http://www.ncbi.nlm.nih.gov/protein/NP_005219.2?ordinalpos=17&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) and nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NG_011529.1?ordinalpos=3&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) information regarding EGFR.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-trastuzumab%20synthesis&cmd=DetailsSearch)]

The synthesis of ^89^Zr-trastuzumab has been described by Dijkers et al. (1). The radiolabeling efficiency for ^89^Zr-trastuzumab was reported to be 77.6 ± 3.9% (n = 3), and the radiochemical purity of the final product was 98.1 ± 1.1% (n = 3) with a specific activity of 67.2 ± 2.4 MBq/mg (1.814 ± 0.064 mCi/mg) (1). For the procedures used to store ^89^Zr-trastuzumab, see Dijkers et al. (1). The labeled mAb was reported to be stable at 4°C with <0.1% degradation/day for up to 7 days. Similarly, the degradation of ^89^Zr-trastuzumab in human serum was <0.5%/day at 37°C for up to 7 days.

For comparative studies, ^111^In-trastuzumab was also produced as described by Dijkers et al. (1). The radiolabeling efficiency and radiochemical purity of this labeled mAb were 89.3 ± 2.1% and 97.0 ± 1.0%, respectively. The specific activity of ^111^In-trastuzumab was 78.2 ± 3.1 MBq/mg (2.11 ± 0.083 mCi/mg) (1), and the stability of ^111^In-labeled trastuzumab was reported to be similar to ^89^Zr-trastuzumab (as given above) at 4°C and 37°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-trastuzumab%20in%20vitro%20studies&cmd=DetailsSearch)]

The in vitro binding characteristics of ^89^Zr-trastuzumab and ^111^In-trastuzumab were determined using SKVO3 cells (human ovarian cancer cell line, overexpressing HER2) and GLC4 cells (human small cell cancer cell line, HER2 negative) by a flow cytometric method (1). Little change in the immunoreactive fraction of ^89^Zr-trastuzumab was noted during 7 days of storage either at 4°C (from 0.87 to 0.85 ± 0.06) or at 37°C in human serum (from 0.87 to 0.78 ± 0.01). A similar trend in the immunoreactivity of ^111^In-trastuzumab was reported at the two storage temperatures.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-trastuzumab%20rodentia&cmd=DetailsSearch)]

Dijkers et al. investigated the biodistribution of ^89^Zr-trastuzumab in athymic mice bearing SKOV3 cell xenograft tumors (n = 5 animals/group) (1). The animals were injected with escalating doses of the radiolabeled mAb (5 MBq ^89^Zr-trastuzumab corresponding to 100, 250, and 500 μg trastuzumab per mouse) through the penile vein, and microPET imaging was performed on the mice on days 1, 3, and 6 after the injection. Although tumor uptake of the label was apparent at 6 h after injection of the radiochemical, the radioactivity was present primarily in the blood at this time point. Subsequently, a decrease in radioactivity in the blood was noted from day 1 to day 6, with a corresponding increase in label in the tumor. Ex vivo analysis of the tissue showed that tumor uptake of the label was similar (30–33% of injected dose/gram tissue (% ID/g); P = 0.75) at the three doses. However, the tumor/blood ratios decreased with increasing doses (7.3, 5.3, and 4.7 at 100, 250, and 500 μg trastuzumab, respectively) and did not differ significantly (P ≥ 0.47) at each dose. Among the various organs examined, maximum uptake of radioactivity was observed in the liver and spleen (9.0% ID/g; both organs have a significant blood supply), and little accumulation of the label was observed in the muscle and brain tissue (<1.0% ID/g). The tumor/liver ratios (3.3, 4.6, and 4.0 at 100, 250, and 500 μg trastuzumab, respectively) did not differ significantly (P ≥ 0.18) at the three injected doses.

Dijkers et al. compared the biodistribution of ^89^Zr-trastuzumab and ^111^In-trastuzumab in athymic mice bearing either SKOV3 or GLC4 xenograft tumors (n = 5 animals/group) (1). The animals were injected with the same respective radiolabeled mAb as before, and accumulation of radioactivity in the various organs was determined at day 1 and day 6 after the injection. Both labeled mAbs had a similar pattern of uptake in the HER2-overexpressing tumors (19.3 ± 2.0% ID/g and 33.4 ± 7.6% ID/g at 1 d and 6 d, respectively, for ^89^Zr-trastuzumab and 17.7 ± 1.9% ID/g and 39.3 ± 9.5% ID/g at 1 d and 6 d, respectively, for ^111^In-trastuzumab; P = 0.47). The HER2-negative tumors had a lower accumulation of radioactivity with both labeled mAbs, with 7.1 ± 0.7% ID/g and 6.8 ± 0.8% ID/g for ^89^Zr-trastuzumab and ^111^In-trastuzumab (P = 0.56), respectively, at day 6 after injection. The amount of label in the blood of mice bearing HER2-positive tumors decreased from 20.4 and 18.6% ID/g for ^89^Zr-trastuzumab and ^111^In-trastuzumab, respectively, at day 1 to 4.3 and 5.3% ID/g, respectively at day 6. The tumor/liver ratios were 5.2 and 7.3 for ^89^Zr-trastuzumab and ^111^In-trastuzumab, respectively, at day 6.

The investigators observed a good correlation (R^2^ = 0.972) in the tumor uptake of both radiobiopharmaceuticals and concluded that, because of its high spatial resolution, ^89^Zr-trastuzumab could be used in the clinical setting after further evaluation.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-trastuzumab%20non%20primate%20mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-trastuzumab%20non%20human%20primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=89Zr-trastuzumab%20human%20studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Dijkers E.C., Kosterink J.G., Rademaker A.P., Perk L.R., van Dongen G.A., Bart J., de Jong J.R., de Vries E.G., Lub-de Hooge M.N. (2009). Development and characterization of clinical-grade 89Zr-trastuzumab for HER2/neu immunoPET imaging. J Nucl Med.
2 Dijkers E.C., de Vries E.G., Kosterink J.G., Brouwers A.H., Lub-de Hooge M.N. (2008). Immunoscintigraphy as potential tool in the clinical evaluation of HER2/neu targeted therapy. Curr Pharm Des.
3 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
4 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.